# ^111^In-Labeled affibody ABY-025 targeting epidermal growth factor receptor 2

Chemical name: | ^111^In-Labeled affibody ABY-025 targeting epidermal growth factor receptor 2
Abbreviated name: | [^111^In]-ABY-025
Synonym:
Agent Category: | Antibody
Target: | Epidermal growth factor receptor 2 (HER2)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-egfr%20antibodies&cmd=DetailsSearch)]

An overexpressed or a mutated transmembrane epidermal growth factor receptor (EGFR; for details regarding this receptor family, see Hollmen and Elenius (1)) that modulates its physiological functions (cell growth, proliferation, migration, etc.) through an intracellular tyrosine kinase (TK) signaling pathway is known to be involved in the development of various cancers (2). As a consequence, one of the strategies used for the in vivo detection (by imaging) or treatment of cancers that are known to involve the EGFR includes the use of anti-EGFR antibodies (Abs) and monoclonal antibodies (mAbs) or their modified derivatives (3, 4). For use as imaging agents, Abs, mAbs, or their derivatives are designed to bind a radionuclide that serves as a source of the detection signal (4). However, their large size (~150 kDa) does not allow Abs and mAbs to penetrate deep into large tumors, and long blood circulating half-life times result in low sensitivity and the generation of a high background during imaging, thereby limiting their use for the detection or radiotherapy of malignant tumors (5, 6). To circumvent the limitations observed with the Abs and the mAbs, many small Ab or mAb derivatives such as the affibody molecules (ABs) have been generated (6, 7). The ABs can be up to ~7 kDa in size and have the same antigen specificity and binding characteristics as the native Ab from which they are derived. Various Abs have been labeled with radionuclides and evaluated for the detection of cancers (7).

The Z_HER2:342_ affibody, which is based on the Z domain of the staphylococcus protein A, is directed against the human EGFR2 (HER2) and has been investigated extensively (5). The non-binding surface domain of Z_HER2:342_ was then altered to make it suitable for chemical synthesis and to enhance the stability and hydrophilicity of the molecule (5). The resulting AB, Z_HER2:2891_, which had 11 surface assessable amino acids substituted in the parent AB, was radioiodinated and shown to have an accumulation of ~10% of the injected activity per gram tissue (% IA/g) in tumors on mice at 4 h after an intravenous injection, indicating that it was a suitable tracer for the detection of malignant tumors in a murine model (8). In an effort to further improve the stability and hydrophilic properties of Z_HER2:2891_, a 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) moiety was conjugated to the unique C-terminal cysteine of the parent AB to generate a second-generation AB designated ABY-025 (5). The new AB was then labeled with ^111^In ([^111^In]-ABY-025) and evaluated for its in vitro cell binding characteristics and for biodistribution and tumor imaging properties in mice bearing xenograft tumors (derived from SKOV-3, a human ovarian adenocarcinoma (http://www.cancer.gov/cancertopics/wyntk/ovary) cell line that expresses the HER2 receptor) (5). These studies were performed to confirm that the various changes made to the native AB to produce ABY-025 had not changed the in vivo accuracy of the second generation AB for the detection of HER2 and also to confirm there was no change in the tumor and normal uptake properties of ABY-025.

### Other sources of information

Human EGFR Gene (http://www.ncbi.nlm.nih.gov/gene/1956) (Gene ID: 1956)

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_005228.3) of human EGFR variant 1

EGFR in OMIM (http://www.ncbi.nlm.nih.gov/omim/131550) (Online Mendelian Inheritance in Man)

EGFR signaling pathways (http://pid.nci.nih.gov/search/pathway_landing.shtml?what=graphic&jpg=on&pathway_id=200131&source=NATURE&output-format=graphic&ppage=1&genes_a=1956) (NCI-Nature Pathways Interaction Database)

Anti-EGFR antibodies (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-EGFR%20antibodies&cmd=DetailsSearch) in PubMed

EGFR tyrosine kinase inhibitors (http://www.ncbi.nlm.nih.gov/pubmed?term=egfr%20tyrosine%20kinase%20inhibitors&cmd=DetailsSearch) in PubMed

Related chapters (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad) in MICAD

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-ABY-025%20synthesis&cmd=DetailsSearch)]

The synthesis of [^111^In]-ABY-025 has been described by Ahlgren et al. (5). The yield of the labeling reaction was >95%. The labeled AB had a specific activity of 15.1 GBq/μmol (407.7 mCi/μmol) with a radiochemical purity of >97% as determined with size-exclusion chromatography. The tracer was reported to be stable for at least 24 h after labeling.

The biodistribution characteristics of [^111^In]-ABY-025 were compared with those of [^111^In]-DOTA-Z_HER2:2395_-C (9) and [^111^In]-DOTA-Z_HER2:342-pep2_ (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=Z-DOTA111In) in mice bearing SKOV-3 cell xenograft tumors (5). However, the radiochemical yield and purity, stability, and specific activity of [^111^In]-DOTA-Z_HER2:2395_-C and [^111^In]-DOTA-Z_HER2:342-pep2_ used for the biodistribution study were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-ABY-025%20in%20vitro&cmd=DetailsSearch)]

The HER2 binding specificity of [^111^In]-ABY-025 was confirmed in an in vitro blocking experiment with SKOV-3 cells, SKBR-3 (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-30&Template=cellBiology) cells (of human breast adenocarcinoma origin and overexpressing HER2), and NCI-N87 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-5822&Template=cellBiology) cells (of human gastric carcinoma origin and expressing normal levels of HER2) using unlabeled ABY-025 (5). Pretreatment of the different cell types with unlabeled ABY-025 was shown to reduce the cell binding of [^111^In]-ABY-025, indicating that the cellular binding of the tracer was specific to HER2.

In another experiment, the different cell lines were exposed to [^111^In]-ABY-025 for 4 h at 4°C, washed with buffer, and incubated at 37°C for >24 h (5). After 24 h, 81.0 ± 2.0%, 76.0 ± 1.0%, and 58.0 ± 1.0% of radioactivity was shown to remain bound to the SKOV-3, NCI-N87, and SKBR-3 cells, respectively. Cell internalization of the radiolabel was determined to be 12.0%, 13.0 ± 1.0%, and 2.5% for the SKOV-3, NCI-N87, and SKBR-3 cells, respectively. The amount of radioactivity bound to all the cell lines remained almost constant from 2 h to 24 h after exposure to the radiochemical.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-ABY-025%20rodentia&cmd=DetailsSearch)]

Ahlgren et al. studied the comparative biodistribution of [^111^In]-ABY-025, [^111^In]-DOTA-Z_HER2:2395_-C, and [^111^In]-DOTA-Z_HER2:342-pep2_ in BALB/c nu/nu mice (n = 4 animals/group) bearing SKOV-3 xenograft tumors (5). The animals were injected intravenously with the respective radiochemicals and euthanized at predetermined time points post-injection (p.i.). At 4 h p.i., all three radiochemicals were reported to have a high accumulation in the tumors (11.0 ± 3.0% IA/g, 11.0 ± 2.0% IA/g, and 14.0 ± 1.0% IA/g for [^111^In]-ABY-025, [^111^In]-DOTA-Z_HER2:2395_-C, and [^111^In]-DOTA-Z_HER2:342-pep2_, respectively) compared with other soft tissues ranging from 0.07 ± 0.01% IA/g (muscle) to 0.93 ± 0.08% IA/g (gastrointestinal tract) for the three tracers. As expected, the kidneys showed very high uptake (ranging from 181.0 ± 17.0% IA/g to 184 ± 48% IA/g for the three radiochemicals) because this is the route of elimination for these labeled compounds. The tumor/muscle ratio was reported to increase from 27.0 ± 7.0 at 0.5 h to 255 ± 51 at 3 days p.i. (compared with ratios ranging from 6.0 ± 1.0 (blood) to 25.0 ± 7.0 (pancreas) at 0.5 h p.i. to 11.0 ± 2.0 (liver) to 474.0 ± 528 (small intestine) at 3 days p.i.).

To investigate the in vivo receptor binding specificity of [^111^In]-ABY-025, the mice were injected subcutaneously with unlabeled His_6_-Z_HER2:342_, the parent AB of ABY-025 (8), 45 min before injecting the radiolabel (5). Tumors from these animals showed a six-fold lower uptake of radioactivity compared with tumors from animals without pretreatment of the unlabeled AB. This indicated that [^111^In]-ABY-025 had a high specificity for binding to the HER2 receptor. The major organs of the animals showed an accumulation of <3%IA/g radioactivity and animals pre-treated with the non-radioactive AB showed an approximate 50% lower uptake of [^111^In]-ABY-025.

Gamma-camera images from mice bearing the SKOV-3 cell tumors were acquired 0.5 h and 4 h after an intravenous injection of [^111^In]-ABY-025 (5). The xenograft tumors were clearly visible in the images acquired at 0.5 h p.i., and the tumor/contralateral thigh ratio was reported to be 7.0 ± 1.0. This ratio was reported to increase to 25.0 ± 12.0 at 4 h p.i., indicating a quick clearance of radioactivity from blood and the other tissues of the animals. Control animals with A431 cell (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1555&Template=cellBiology) xenograft tumors (derived from a human epidermoid carcinoma; does not express HER2) did not show any uptake of radioactivity.

Groups of rats (n = 8 animals per group) given five consecutive injections of three different doses of ABY-025 (2, 6, and 30 μg, respectively) every 3 weeks did not develop any immunogenicity against the AB (5). Only 1 of 24 animals showed a very low-level immune response after the second injection, and the antibody level remained almost constant even after the three additional treatments of ABY-025. This indicated that the AB was not immunogenic in rats at the doses used for the study.

In another study, the pharmacokinetics of [^111^In]-ABY-025 was investigated in rats (n = 3 animals/gender) (5). Each animal was intravenously administered the tracer at a dose of 0.424 mg/kg body weight (2.0 kBq/μg (54 pCi/μg)), and blood samples were taken from the animals at fixed time points ranging from 2 min to 240 min. A biphasic decrease in concentration of the label was observed in both genders of the rats, and the mean initial and terminal half-lives in the animals were determined to be 9–14 min and 52–58 min, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-ABY-025%20non-primate%20mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-ABY-025%20non-human%20primates&cmd=DetailsSearch)]

The pharmacokinetics of [^111^In]-ABY-025 were also investigated in cynomolgus macaques (Macaca fascicularis; n = 3 animals/gender) (5). The tracer was administered at a dose of 0.424 mg/kg body weight (1.6 kBq/μg (43.5 pCi/μg)), and blood samples were taken as described for the rat study above. Similar to the rats, a biphasic decrease in the concentration of the tracer was observed in the macaques, and the mean initial and terminal half-lives were determined to be 12–19 min and 104–123 min, respectively, in these animals.

From the various studies performed with [^111^In]-ABY-025, the investigators concluded that the radiochemical can be used for the detection of HER2-expressing xenograft tumors in a murine model. In addition, the AB was suitable for further development because it did not evoke an immune response in rats and macaques (5).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-ABY-025%20Humans&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Hollmen M., Elenius K. (2010). Potential of ErbB4 antibodies for cancer therapy. Future Oncol.
2 Friedman M., Lindstrom S., Ekerljung L., Andersson-Svahn H., Carlsson J., Brismar H., Gedda L., Frejd F.Y., Stahl S. (2009). Engineering and characterization of a bispecific HER2 x EGFR-binding affibody molecule. Biotechnol Appl Biochem.
3 Huang L., De Baetselier P., Beyaert R. (2009). Targeting the EGF receptor ectodomain in the context of cancer. Expert Opin Ther Targets.
4 Mishani E., Abourbeh G., Eiblmaier M., Anderson C.J. (2008). Imaging of EGFR and EGFR tyrosine kinase overexpression in tumors by nuclear medicine modalities. Curr Pharm Des.
5 Ahlgren S., Orlova A., Wallberg H., Hansson M., Sandstrom M., Lewsley R., Wennborg A., Abrahmsen L., Tolmachev V., Feldwisch J. (2010). Targeting of HER2-expressing tumors using 111In-ABY-025, a second-generation affibody molecule with a fundamentally reengineered scaffold. J Nucl Med.
6 Lofblom J., Feldwisch J., Tolmachev V., Carlsson J., Stahl S., Frejd F.Y. (2010). Affibody molecules: engineered proteins for therapeutic, diagnostic and biotechnological applications. FEBS Lett.
7 Ahlgren, S. and V. Tolmachev, Radionuclide Molecular Imaging using Affibody Molecules. Curr Pharm Biotechnol, 2010
8 Orlova A., Magnusson M., Eriksson T.L., Nilsson M., Larsson B., Hoiden-Guthenberg I., Widstrom C., Carlsson J., Tolmachev V., Stahl S., Nilsson F.Y. (2006). Tumor imaging using a picomolar affinity HER2 binding affibody molecule. Cancer Res.
9 Ahlgren S., Orlova A., Rosik D., Sandstrom M., Sjoberg A., Baastrup B., Widmark O., Fant G., Feldwisch J., Tolmachev V. (2008). Evaluation of maleimide derivative of DOTA for site-specific labeling of recombinant affibody molecules. Bioconjug Chem.